# ^68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-cyclo(Arg-Gly-Asp-D-Phe-Lys)

Chemical name: | ^68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-cyclo(Arg-Gly-Asp-D-Phe-Lys)
Abbreviated name: | ^68^Ga-DOTA-E-c(RGDfK)
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Dijkgraaf et al. (13) reported the development of ^111^In-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-cyclo(Arg-Gly-Asp-D-Phe-Lys) (^111^In-DOTA-E-c(RGDfK)) for single-photon emission computed tomography imaging α_v_β_3_ receptors in nude mice bearing ovarian carcinoma tumors. In this chapter, Dijkgraaf et al. (14) also reported the evaluation of ^68^Ga-DOTA-E-c(RGDfK) for positron emission tomography (PET) imaging α_v_β_3_ receptors in tumor, which is the topic of this chapter.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+synthesis)]

Dijkgraaf et al. (14) prepared the synthesis of ^68^Ga-DOTA-E-c(RGDfK) by reacting DOTA-E-c(RGDfK) with ^68^Ga in ammonium acetate buffer (pH ~5.5) at 95°C for 20 min. Radiochemical purity was ~97% as determined by high-performance liquid chromatography. The maximum specific activity was 11.2 MBq/nmol (0.3 mCi/nmol). ^68^Ga-DOTA-E-c(RGDfK) was stable in phosphate-buffered saline and human serum at 37°C for 2 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+in+vitro)]

Dijkgraaf et al. (14) performed in vitro solid-phase binding assays of ^111^In-DOTA-E-[c(RGDfK)]_2_ with human α_v_β_3_ integrin. ^nat^Ga-DOTA-E-c(RGDfK) (monomer) had an IC_50_ value of 23.9 ± 1.22 nM. ^nat^Ga-DOTA-E-[c(RGDfK)]_2_ (dimer) had an IC_50_ value of 8.99 ± 1.20 nM. ^nat^Ga-DOTA-E-{E-[c(RGDfK)]_2_}_2_ (tetramer) had an IC_50_ value of 1.74 ± 1.18 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+rodentia)]

Dijkgraaf et al. (14) performed ex vivo biodistribution studies of ^68^Ga-DOTA-E-c(RGDfK) in nude mice (n = 3/group) bearing SK-RC-52 human renal carcinoma tumors at 2 h after injection. The tumor accumulation was 3.3 ± 0.3% injected dose/gram (ID/g). The organ with the highest accumulation was the intestine (~4% ID/g), followed by the spleen (~2.5% ID/g), kidney (~2.5% ID/g), liver (~2.0% ID/g) and colon (~2.0% ID/g). Coinjection of 100-fold excess DOTA-E-[c(RGDfK)]_2_ resulted in >90% reduction of radioactivity in the tumor. The accumulation was also markedly reduced in the liver, lung, intestine, colon and spleen (this may be partly mediated by α_v_β_3_ integrin in these tissues) but not in the kidney. PET scan showed that the tumor was clearly visualized at 2 h after injection of 10 MBq (0.27 mCi) ^68^Ga-DOTA-E-c(RGDfK).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Dijkgraaf I., Kruijtzer J.A., Frielink C., Corstens F.H., Oyen W.J., Liskamp R.M., Boerman O.C. (2007). Alpha v beta 3 integrin-targeting of intraperitoneally growing tumors with a radiolabeled RGD peptide. Int J Cancer.
14 Dijkgraaf I., Yim C.B., Franssen G.M., Schuit R.C., Luurtsema G., Liu S., Oyen W.J., Boerman O.C. (2011). PET imaging of alphavbeta integrin expression in tumours with Ga-labelled mono-, di- and tetrameric RGD peptides. Eur J Nucl Med Mol Imaging.